# ^64^Cu-Labeled 4-((8-amino-3,6,10,13,16,19-hexaazabicyclo [6.6.6] icosane-1-ylamino)methyl)benzoic acid (AmBaSar)

Chemical name: | ^64^Cu-Labeled 4-((8-amino-3,6,10,13,16,19-hexaazabicyclo [6.6.6] icosane-1-ylamino)methyl)benzoic acid (AmBaSar)
Abbreviated name: | [^64^Cu]-AmBaSar
Synonym:
Agent Category: | Compound
Target: | Non-targeted
Target Category:
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure of [^64^Cu]-AmBaSar for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu%20AmBaSar&cmd=DetailsSearch)]

Radionuclides such as ^18^F, ^11^C, ^124^I, ^64^Cu, etc., are often used to label molecular imaging probes (MIP) for positron emission tomography (PET) of patients to detect and diagnose a variety of diseases, including cancer (1). However, some limitations (to mention a few) for the production and application of these MIPs are a short half-life (e.g., 110 min and 12 min for ^18^F and ^11^C, respectively), production of low quality images (e.g., with ^124^I), high radiation doses (e.g., ^66^Ga and ^76^Br), and accumulation in the liver or kidneys due to metabolic degradation (e.g., ^64^Cu) (1). In addition, MIPs labeled with nuclides that have a short half-life cannot be used in cases where long circulation times are necessary to obtain an optimal target/background signal. The limitations of various nuclides evaluated for the production and application of different PET MIPs are discussed in detail by Nayak and Brechbiel (1). Some investigators are particularly interested in the use of ^64^Cu to produce PET imaging probes because ^64^Cu is suitable as a source of the signal, it is relatively easily obtained, and its nuclear properties make it an excellent therapeutic radionuclide (t_1/2_ = 12.7 h; β^+^: 17.4%; E_β+_max = 656 keV; β: 39%; E_β-_max = 573 keV) (2). Linking ^64^Cu to MIPs requires the use of a bifunctional chelator (BFC) that connects the radionuclide to the targeted probe. Therefore, it is important to have an appropriate BFC to create a ^64^Cu-labeled radiopharmaceutical that remains stable under in vivo conditions and generates suitable results during PET imaging.

Several types of chelating agents have been used for the ^64^Cu-labeling of imaging probes, but some of the limitations for using these radiochemicals in humans include poor yields due to complicated procedures for the synthesis, harsh conditions used to label the compound that can degrade a probe, in vivo instability, lack of sufficient biological data, and accumulation in non-targeted organs that results in the masking of small lesions during PET imaging (3). In an effort to create a BFC that could be synthesized and labeled easily with ^64^Cu, a sarcophagine-based chelator, 4-((8-amino-3,6,10,13,16,19-hexaazabicyclo [6.6.6] icosane-1-ylamino)methyl)benzoic acid (AmBaSar), was produced by Cai et al. (2). A characteristic feature of this BFC is that it can rapidly form a coordination complex with metal ions within a cage-like structure that does not dissociate under physiological conditions. o further simplify the synthesis of AmBaSar, the investigators devised a four-step procedure to label the chelator with ^64^Cu ([^64^Cu]-AmBaSar) (3). [^64^Cu]-AmBaSar was then evaluated for its in vitro stability, microPET imaging characteristics, and biodistribution in normal mice (3). In addition, the stability, imaging, and biodistribution properties of [^64^Cu]-AmBaSar were compared with those of ^64^Cu-labeled 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid ([^64^Cu]-DOTA). In an earlier study AmBaSar was linked to Arg-Gly-Asp (RGD), a cyclic peptide that specifically binds to the α_v_β_3_ integrin receptor, and labeled it with ^64^Cu to obtain [^64^Cu]-AmBaSar-RGD (2). Subsequently the labeled RGD complex was shown to be suitable for the detection of tumors expressing α_v_β_3_ integrin receptors in mice. Studies performed with [^64^Cu]-AmBaSar-RGD are described in a separate chapter of MICAD (www.micad.nih.gov) (4).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu%20AmBaSar%20synthesis&cmd=DetailsSearch)]

The simplified synthesis of AmBaSar and its labeling with ^64^Cu have been described by Cai et al. (3). The radiochemical yield of [^64^Cu]-AmBaSar was reported to be >95% as determined with radiographic thin-layer chromatography (radio-TLC). During TLC analysis, the R_f_ value of [^64^Cu]-AmBaSar was determined to be 0.71 (close to the solvent front), whereas the unbound ^64^Cu remained at the origin. The radiochemical purity of the tracer was >95% as determined with radiographic high-performance liquid chromatography (radio-HPLC). The specific activity of the labeled compound was not reported.

For comparison purposes, [^64^Cu]-DOTA was also synthesized and used in some studies (3). This tracer had a radiochemical yield of >98%; however, its radiochemical purity and specific activity were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu%20AmBaSar%20in%20vitro&cmd=DetailsSearch)]

Using a 1-octanol/water system, the partition coefficients of [^64^Cu]-AmBaSar and [^64^Cu]-DOTA were reported to be −2.6 and −2.3, respectively, indicating that both radiocompounds had a hydrophilic nature (3).

The in vitro stability of [^64^Cu]-AmBaSar was determined by exposing the labeled compound to phosphate-buffered saline (PBS; pH 7.4), fetal bovine serum (FBS), and mouse blood, respectively (3). The radiochemical had a stability of >97% for up to 26 h in PBS and FBS as determined with radio-HPLC. When incubated with mouse blood, the tracer was reported to have a stability of >98% for up to 4 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu%20AmBaSar%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^64^Cu]-AmBaSar was studied in normal mice (n = 3 animals) and compared with that of [^64^Cu]-DOTA in the same number of animals (3). The tracers were administered intravenously to the animals, and the mice were euthanized 2 h later to determine the amount of radioactivity accumulated in the major organs. Data obtained from this study were presented as percent of injected dose per gram of tissue (% ID/g). At 2 h after injection of [^64^Cu]-AmBaSar, the uptake of radioactivity in the liver and kidneys was 0.14 ± 0.01%ID/g and 1.09 ± 0.27% ID/g, respectively, indicating that the label was cleared from these animals mainly through the urinary route. With [^64^Cu]-DOTA, the accumulation of radioactivity in the kidneys and the liver was 1.28 ± 0.41% ID/g and 1.25 ± 0.09% ID/g, respectively, during the same period, suggesting that this radiochemical was cleared almost equally through the urinary and hepatobiliary routes in these animals.

MicroPET images were acquired from mice (n = 2 animals/tracer) at 30 min and 2 h after intravenous injection of either [^64^Cu]-AmBaSar or [^64^Cu]-DOTA (3). With [^64^Cu]-AmBaSar, the radioactivity accumulated mainly in the kidneys and the bladder at 30 min after injection; with [^64^Cu]-DOTA, radioactivity was present primarily in the liver, kidneys, and the bladder at this time point. With both radiochemicals, most of the radioactivity cleared through the bladder by 2 h after injection, but residual radioactivity was still evident in the liver and bowels of animals that received [^64^Cu]-DOTA. The imaging study confirmed the results obtained from the biodistribution study.

From these studies, the investigators concluded that AmBaSar was suitable for the preparation of ^64^Cu-labeled radiochemicals and their use as imaging agents in rodents (3).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu%20AmBaSar%20non-primate%20mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu%20AmBaSar%20non-human%20primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu%20AmBaSar%20humans&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Nayak T.K., Brechbiel M.W. (2009). Radioimmunoimaging with longer-lived positron-emitting radionuclides: potentials and challenges. Bioconjug Chem.
2 Cai H., Fissekis J., Conti P.S. (2009). Synthesis of a novel bifunctional chelator AmBaSar based on sarcophagine for peptide conjugation and (64)Cu radiolabelling. Dalton Trans.
3 Cai H., Li Z., Huang C.W., Park R., Shahinian A.H., Conti P.S. (2010). An improved synthesis and biological evaluation of a new cage-like bifunctional chelator, 4-((8-amino-3,6,10,13,16,19-hexaazabicyclo[6.6.6]icosane-1-ylamino)methyl) benzoic acid, for 64Cu radiopharmaceuticals. Nucl Med Biol.
4 Chopra, A., [64Cu]-Labeled 4-((8-amino-3,6,10,13,16,19-hexaazabicyclo [6.6.6] icosane-1-ylamino) methyl) benzoic acid (AmBaSar) conjugated to cyclic arginine-glycine-aspartic acid (RGD) peptide. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.